# ^124^I-Labeled residulizing ligand IMP-R4 conjugated chimeric monoclonal antibody ch806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)

Chemical name: | ^124^I-Labeled residulizing ligand IMP-R4 conjugated chimeric monoclonal antibody, ch806, targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Abbreviated name: | [^124^I]-IMP-R4-ch806
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Target Category: | Receptor
Method of detection: | Positron emission tomography
Source of signal / contrast: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, and functioning of the different members of the transmembrane epidermal growth factor receptor (EGFR) family are described elsewhere (1-3). These receptors are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (1, 2). Overexpression of the EGFR in the tumors has been attributed to gene amplification, and this phenomenon is believed to introduce mutations in the receptor (2, 4). Also, overexpression of the EGFR usually indicates a poor clinical prognosis for the patient (4). The most common mutation observed in the receptor is the deletion of a segment of the EGFR extracellular domain, including the ligand-binding region, which results in the generation of a variant known as the de2-7 EGFR or EGFRvIII (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy have been reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to the ligand, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain the cancerous state of cells, several antibodies that inhibit the receptor activity and small molecules that block the downstream TK signaling pathway have been developed and have been approved by the United States Food and Drug Administration (FDA) for the treatment of certain cancers (2). The antibodies are directed toward the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which ultimately results in downregulation of the EGFR on the cell surface. However, because the EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). As a consequence, the monoclonal antibody (mAb) 806, which specifically targets the EGFRvIII, was generated and characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated as ch806, was developed and evaluated in a phase I clinical trial with patients having cancerous tumors overexpressing the EGFRvIII (4). Results obtained from this trial indicated that ch806 could be a good biotherapeutic agent for the treatment of cancers expressing the ch806 antigen (4). In addition, several other clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) approved by the FDA are in progress to evaluate the targeting of EGFRvIII as a treatment against various cancers.

The internalization, intracellular trafficking, and biodistribution (in nude mice bearing xenograft human epidermoid carcinoma cell tumors) of mAb806 labeled with ^125^I and ^111^In, respectively, are described in separate chapters (9, 10) in MICAD (www.micad.nih.gov). The characterization and biodistribution (in nude mice bearing xenograft human glioblastoma cell tumors) of chb806 labeled with ^125^I or ^111^In are also described in separate chapters (11, 12) in MICAD. This chapter describes the evaluation of ^124^I-labeled ch806 ([^124^I]-ch806) for the detection of EGFRvIII-expressing xenograft human glioblastoma tumors in nude mice using an immuno–positron emission tomography (PET) technique as reported by Lee et al. (6). The biodistribution of the radiolabeled chimeric antibody was also studied in the tumor-bearing animals.

### Other sources of information

Human EGFR Gene (http://www.ncbi.nlm.nih.gov/gene/1956) (Gene ID: 1956)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200131&source=NATURE&output-format=graphic&ppage=1&genes_a=1956) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20synthesis&cmd=DetailsSearch)]

The synthesis of [^124^I]-ch806 was described by Lee et al. (6). Briefly, labeling of ch806 with ^124^I was performed after conjugation of the chAb to IMP-R4, a residualizing ligand, to obtain [^124^I]-IMP-R4-ch806. IMP-R4 is MCC-Lys(MCC)-Lys(X)-D-Tyr-D-Lys(X)-OH, where MCC is 4-(N-maleimidomethyl)-cyclohexane-1-carbonyl and X is 1-[(4-thiocarbonylamino)benzyl]-diethylenetriamine pentaacetic acid. The labeling efficiency of the reaction was reported to be 51.2%, and 96.6% of the radioactivity was bound to the protein as determined with thin-layer chromatography. The radiochemical purity of the labeled chAb was not reported. The specific activity of [^124^I]-IMP-R4-ch806 was reported to be 1.961 MBq/6.6 pmol (~ 8,030 Ci/mmol). The number of IMP-R4 moieties bound per molecule of ch806, and the final formulation and storage conditions of the labeled chAb were not reported.

For use as controls, ch806 and another mAb, huA33 (a humanized mAb that targets the A33 antigen), were also labeled with ^124^I (6). The characteristics and cell-binding properties of these labeled antibodies are described by Lee et al. (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20in%20vitro&cmd=DetailsSearch)]

With the use of the Lindmo assay, the immunoreactivity of [^124^I]-IMP-R4-ch806 to U97MG.de2-7 cells, which express the EGFRvIII receptor, was reported to be 78.3% (6). The apparent association constant of [^124^I]-IMP-R4-ch806 (determined in the presence of unlabeled ch806 using a Scatchard plot) and the number of chAb molecules bound per cell were reported to be 5.6 × 10^8^ M^–1^ and 1.12 × 10^6^, respectively (6).

The stability of [^124^I]-IMP-R4-ch806 on day 3 and day 7 after labeling was 52.1% and 34.3%, respectively, as determined with an immunoreactive assay (described above) and high-performance liquid chromatography analysis of the samples (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^124^I]-IMP-R4-ch806 was studied in BALB/c nude mice bearing xenograft U97MG.de2-7 cell tumors (6). The animals (n = 5 animals/time point) were injected with the labeled antibody through the tail vein, and the mice were euthanized at different time points for the collection of all major organs, including the tumors (6). The tumors had a maximum accumulation of radioactivity of 30.95 ± 6.01% injected dose per gram tissue (% ID/g) at 48 h post-injection (p.i.), which decreased to 14.64 ± 2.52% ID/g by 120 h p.i. [^111^In]-chAb806 peaked at ~31.0% ID/g at 48 h.The tumor/blood ratios were reported to increase from 0.45 ± 0.07% ID/g at 4 h p.i. to 5.25 ± 2.45% ID/g at 120 h p.i., and a similar trend in radioactivity uptake was noted in the normal tissues. Compared to [^124^I]-IMP-R4-ch806, low levels of radioactivity (ranging from ~5% to 7.00% ID/g) were detected in the tumors with the control ^124^I-labeled antibodies (6). No blocking studies using unlabeled ch806 were reported.

PET/computed tomography (CT) imaging was performed at 4, 24, 48, and 168 h p.i. (n = 2 mice/time point) (6). The tumor uptake of radioactivity was clearly evident at 24 h p.i. and was reported to increase with time, remaining visible up to 168 h p.i. The pattern of radioactivity uptake by the normal tissues observed with PET/CT imaging was similar to that observed during the biodistribution studies. No blocking studies were performed.

From these studies, the investigators concluded that immuno-PET with [^124^I]-IMP-R4-ch806 can be used for the detection of tumors overexpressing EGFRvIII in mice (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Hasselbalch, B., U. Lassen, H.S. Poulsen, and M.T. Stockhausen, Cetuximab Insufficiently Inhibits Glioma Cell Growth Due to Persistent EGFR Downstream Signaling. Cancer Invest. 2010
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Chopra, A., [125I]-Labeled monoclonal antibody 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated monoclonal antibody 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., [125I]-Labeled chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.